# [^11^C]Acetate

Chemical name: | [^11^C]Acetate
Abbreviated name:
Synonym: | [^11^C]Acetic acid
Agent Category: | Compound
Target: | TCA cycle, fatty acid synthetase,
Target Category: | Incorporation into membrane
Method of detection: | PET
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate mammals; - Non-human primates; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%22carbon-11%20acetate%22%5BSubstance%20Name%5D%20OR%2011C%5BAll%20Fields%5D%20AND%20acetate%5BText%20Word%5D%29)]

Acetate is readily taken up by cells and is activated to acetyl-CoA in both the cytosol and mitochondria by acetyl-CoA synthetase. Acetyl-CoA is a common metabolic intermediate for synthesis of cholesterol and fatty acids, which are then incorporated into membrane (1). Acetyl-CoA is also oxidized in mitrochondria by the tricarboxylic acid (TCA) cycle to carbon dioxide and water. Some of the acetate is converted to amino acids. In normal myocardium, acetate is metabolized to CO_2_ via the TCA cycle as the dominant pathway. In contrast, tumor cells convert most of the acetate into fatty acids by a key enzyme fatty acid synthetase (FAS), which is over-expressed in cancer cells (2). Acetate is predominantly incorporated into intracellular phosphatidylcholine membrane microdomains that are important for tumor growth and metastasis (3). [^11^C]Acetate are used as a positron emission tomography (PET) tracer for studying myocardial oxidative metabolism and regional myocardial blood flow (4). [^11^C]Acetate is a promising PET tracer for renal, pancreatic, and prostate tumors (5).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%22carbon-11%20acetate%22%5BSubstance%20Name%5D%20OR%2011C%5BAll%20Fields%5D%20AND%20acetate%5BText%20Word%5D%29%20AND%20synthesis)]

[^11^C]Acetate is commonly produced by a reaction of methylmagnesium bromide or chloride and [^11^C]carbon dioxide. This method produces [^11^C]acetate in a radiochemical yield of 72 ± 12% in 20 min and in high specific activity (>18.5 GBq/µmol, 0.5 Ci/µmol). The radiochemical purity of [^11^C]acetate was found to be > 95% (6). Several automated systems provided radiochemical yields of 60 - 80% and radiochemical purity of 99% in 15 - 23 min (7-9)

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%22carbon-11%20acetate%22%5BSubstance%20Name%5D%20OR%2011C-acetate%5BText%20Word%5D%29%20AND%20%22in%20vitro%22%5BMeSH%20Terms%5D)]

Acetate uptake and metabolism were studied in four tumor cell lines and one fibroblast cell line with [^14^C]acetate. All four tumor cell lines showed higher accumulation of [^14^C] activity than the resting fibroblasts. Tumor-to-fibroblast ratios were larger than those of [^3^H]-2-deoxyglucose. [^14^C]Acetate was metabolized and incorporated into phosphatidylcholine and neutral lipids in proportionally to cellular proliferation rates. The remaining fraction of [^14^C]acetate was converted to amino acids, acetylCoA, and CO_2_ (10). This was shown by extraction of tissue samples followed by analysis using thin layer chromatography and paper chromatography with authentic samples of possible metabolites.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%22carbon-11%20acetate%22%5BSubstance%20Name%5D%20OR%201-11C-acetate%5BText%20Word%5D%29%20AND%20%28%22rodentia%22%5BMeSH%20Terms%5D%20OR%20rodentia%5BText%20Word%5D%29)]

Tissue accumulation of [^11^C]acetate was studied in mice with EMT-6 murine mammary carcinoma tumors and rats with 9L-glioma tumors at 1 h postinjection of the tracer (11). In the EMT-6 mice, the organ with the highest uptake was in the pancreas (2.49% injected dose/g (ID/g)), followed by the liver (1.42% ID/g), spleen (1.40% ID/g) and kidneys (1.18% ID/g). The tumor uptake was only 0.60% ID/g giving a tumor-to-blood ratio of 1.3. In the rats bearing 9L-glioma tumors, the organ with the highest uptake was in the pancreas (0.88% ID/g), followed by the spleen (0.42% ID/g), liver (0.35% ID/g), and kidneys (0.33% ID/g). The tumor uptake was only 0.42% ID/g giving a tumor-to-blood ratio of 3.2.

Oyama et al. reported that androgen ablation caused a decrease of 2-[^18^F] fluoro-2-deoxy-D-glucose ([^18^F]FDG) and [^11^C]acetate uptake in the prostate in Sprague-Dawley male rats to monitor metabolic changes in normal prostate tissue. Dihydrotestosterone administration returned uptake of both tracers to that of the baseline level. Therefore, serum testosterone levels influence glucose and acetate metabolism in the prostate (12).

[^11^C]Acetate has been used to study myocardial oxygen consumption rate (MVO_2_) with the metabolic fate of the tracer in normoxic, hypoxic, and ischemic conditions in isolated perfused rat hearts. Model-estimated MVO_2_ correlated well with experimentally measured MVO_2_ for these conditions correlated strongly with the myocardial clearance rate determined from the tissue kinetics (13).

In a rat model of an occluded, acute left anterior descending (LAD) coronary artery, ^60^Cu-ATSM was used to visualize hypoxic rat heart tissue using an ex vivo tissue slice imaging technique (14). In addition, [^11^C]acetate was used to monitor myocardial blood flow. Low [^11^C]acetate uptake (low blood flow) and high ^60^Cu-ATSM uptake (hypoxia) were observed in mildly ischemic regions. In the center of severely ischemic regions with no blood flow, little accumulation of ^11^C or ^60^Cu radioactivity was observed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=1-11C-acetate%5BText%20Word%5D%20AND%20%22animals%22%5BMeSH%5D%20NOT%20%22rodentia%22%5BMeSH%20Terms%5D%20NOT%20%22primates%22%5BMeSH%5D)]

[^11^C]Acetate PET was used to study cardiac output in a pig model (15). The tracer uptake in the right and left heart cavities was measured as well as in the lung. Myocardial output measured by [^11^C]acetate PET was linearly related to cardiac output by thermodilution. Lung uptake of [^11^C]acetate was also linearly related to stroke volume.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%22carbon-11%20acetate%22%5BSubstance%20Name%5D%20OR%2011C-acetate%5BText%20Word%5D%29%20AND%20%22primates%22%5BMeSH%5D%20NOT%20%22humans%22%5BMeSH%5D)]

[^11^C]Acetate PET was studied in monkeys with coronary ligation. The infract myocardial regions showed a decrease in tracer accumulation (16).

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%22carbon-11%20acetate%22%5BSubstance%20Name%5D%20OR%201-11C-acetate%5BText%20Word%5D%29%20AND%20%22humans%22%5BMeSH%20Terms%5D)]

Myocardial oxygen consumption can be estimated with PET from analysis of the myocardial turnover rate constant (k) after administration of [^11^C]acetate. [^11^C]Acetate was administered to five normal volunteers and six patients with myocardial infarction. Uptake of [^11^C]acetate by the myocardium was avid, and its clearance from the blood pool was rapid, yielding myocardial images of excellent quality. Regional k was homogeneous in the myocardiums of healthy volunteers. In patients, k in regions remote from the area of infarction was not different from values in the myocardiums of healthy human volunteers. In contrast, k in the center of the infarct region of necrotic myocardium was significantly reduced (17).

[^11^C]Acetate PET has been shown to have high sensitivity for detection of recurrent prostate cancer and metastases. It was reported that 27 of 46 prostate cancer patients were positive with [^11^C]acetate PET studies, whereas only eight [^18^F]FDG PET studies had positive detections (18). In another study, it was cautioned that acetate also accumulates in normal, hyperplastic, and benign prostate tissues. It was reported that the [^11^C]acetate standardized uptake values for normal prostate and benign prostate, overlap significantly with those for prostate cancer patients (19).

Human dosimetry was estimated in six healthy volunteers by intravenous injection of 525 MBq (14.2 mCi) of [^11^C]acetate (20). The organs receiving the highest absorbed doses were the pancreas (0.017 mGy/MBq or 62.9 mrad/mCi), bowel (0.011 mGy/MBq or 40.7 mrad/mCi), kidneys (0.0092 mGy/MBq or 34.0 mrad/mCi), and spleen (0.0092 mGy/MBq or 34.0 mrad/mCi). No urinary excretion of tracer was detected. The effective dose equivalent was 0.0062 mSv/MBq (22.9 mrem/mCi).

[^11^C]Acetate is rapidly taken up by myocardium and metabolized to CO_2_ and water after intravenous injection. The uptake is indirectly dependent on blood flow (21). The clearance of the tracer is a direct reflection of TCA cycle activity, which is coupled to myocardial oxygen consumption [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%22carbon-11%20acetate%22%5BSubstance%20Name%5D%20OR%201-11C-acetate%5BText%20Word%5D%29%20AND%20%22humans%22%5BMeSH%5D%20AND%20mvo2%5BAll%20Fields%5D)]. Rates of clearance from myocardium of [^11^C]acetate reflect oxidative metabolism (22). [^11^C]Acetate PET is used to evaluate ischemia and myocardial infraction [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%22carbon-11%20acetate%22%5BSubstance%20Name%5D%20OR%201-11C-acetate%5BText%20Word%5D%29%20AND%20%22humans%22%5BMeSH%5D%20AND%20%22myocardium%22%5BMeSH%20Terms%5D)]. Many prostate, bladder, and renal cancer patients have been imaged with [^11^C]acetate PET to assess primary and metastatic tumors [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%22carbon-11%20acetate%22%5BSubstance%20Name%5D%20OR%201-11C-acetate%5BText%20Word%5D%29%20AND%20%22humans%22%5BMeSH%20Terms%5D%20AND%20%22neoplasms%22%5BMeSH%20Terms%5D)].

## NIH Support

HL13851, P30 CA91842, R24 CA83060, HL29845, HL33177, HL17646, R01 HL46895, R01 HL58408, RR00645

## References

1 Howard B.V., Howard W.J. (1975). Lipids in normal and tumor cells in culture. Prog Biochem Pharmacol.
2 Swinnen J.V., Heemers H., Deboel L., Foufelle F., Heyns W., Verhoeven G. (2000). Stimulation of tumor-associated fatty acid synthase expression by growth factor activation of the sterol regulatory element-binding protein pathway. Oncogene.
3 Swinnen J.V., Van Veldhoven P.P., Timmermans L., De Schrijver E., Brusselmans K., Vanderhoydonc F., Van de Sande T., Heemers H., Heyns W., Verhoeven G. (2003). Fatty acid synthase drives the synthesis of phospholipids partitioning into detergent-resistant membrane microdomains. Biochem Biophys Res Commun.
4 Visser F.C. (2001). Imaging of cardiac metabolism using radiolabelled glucose, fatty acids and acetate. Coron Artery Dis.
5 Schoder H., Larson S.M. (2004). Positron emission tomography for prostate, bladder, and renal cancer. Semin Nucl Med.
6 Pike V.W., Eakins M.N., Allan R.M., Selwyn A.P. (1982). Preparation of [1-11C]acetate--an agent for the study of myocardial metabolism by positron emission tomography. Int J Appl Radiat Isot.
7 Kruijer P.S., Ter Linden T., Mooij R., Visser F.C., Herscheid J.D.M. (1995). A practical method for the preparation of [11C]acetate. Appl. Radiat. Isot.
8 Moerlein S.M., Gaehle G.G., Welch M.J. (2002). Robotic preparation of Sodium Acetate C 11 Injection for use in clinical PET. Nucl Med Biol.
9 Roeda D., Dolle F., Crouzel C. (2002). An improvement of 11C acetate synthesis--non-radioactive contaminants by irradiation-induced species emanating from the 11C carbon dioxide production target. Appl Radiat Isot.
10 Yoshimoto M., Waki A., Yonekura Y., Sadato N., Murata T., Omata N., Takahashi N., Welch M.J., Fujibayashi Y. (2001). Characterization of acetate metabolism in tumor cells in relation to cell proliferation: acetate metabolism in tumor cells. Nucl Med Biol.
11 Jonson S.D., Welch M.J. (2002). Investigations into tumor accumulation and peroxisome proliferator activated receptor binding by F-18 and C-11 fatty acids. Nucl Med Biol.
12 Oyama N., Kim J., Jones L.A., Mercer N.M., Engelbach J.A., Sharp T.L., Welch M.J. (2002). MicroPET assessment of androgenic control of glucose and acetate uptake in the rat prostate and a prostate cancer tumor model. Nucl Med Biol.
13 Ng C.K., Huang S.C., Schelbert H.R., Buxton D.B. (1994). Validation of a model for [1-11C]acetate as a tracer of cardiac oxidative metabolism. Am J Physiol.
14 Fujibayashi Y., Cutler C.S., Anderson C.J., McCarthy D.W., Jones L.A., Sharp T., Yonekura Y., Welch M.J. (1999). Comparative studies of Cu-64-ATSM and C-11-acetate in an acute myocardial infarction model: ex vivo imaging of hypoxia in rats. Nucl Med Biol.
15 Sorensen J., Stahle E., Langstrom B., Frostfeldt G., Wikstrom G., Hedenstierna G. (2003). Simple and accurate assessment of forward cardiac output by use of 1-(11)C-acetate PET verified in a pig model. J Nucl Med.
16 Norol F., Merlet P., Isnard R., Sebillon P., Bonnet N., Cailliot C., Carrion C., Ribeiro M., Charlotte F., Pradeau P., Mayol J.F., Peinnequin A., Drouet M., Safsafi K., Vernant J.P., Herodin F. (2003). Influence of mobilized stem cells on myocardial infarct repair in a nonhuman primate model. Blood.
17 Walsh M.N., Geltman E.M., Brown M.A., Henes C.G., Weinheimer C.J., Sobel B.E., Bergmann S.R. (1989). Noninvasive estimation of regional myocardial oxygen consumption by positron emission tomography with carbon-11 acetate in patients with myocardial infarction. J Nucl Med.
18 Oyama N., Miller T.R., Dehdashti F., Siegel B.A., Fischer K.C., Michalski J.M., Kibel A.S., Andriole G.L., Picus J., Welch M.J. (2003). 11C-acetate PET imaging of prostate cancer: detection of recurrent disease at PSA relapse. J Nucl Med.
19 Kato T., Tsukamoto E., Kuge Y., Takei T., Shiga T., Shinohara N., Katoh C., Nakada K., Tamaki N. (2002). Accumulation of [11C]acetate in normal prostate and benign prostatic hyperplasia: comparison with prostate cancer. Eur J Nucl Med Mol Imaging.
20 Seltzer M.A., Jahan S.A., Sparks R., Stout D.B., Satyamurthy N., Dahlbom M., Phelps M.E., Barrio J.R. (2004). Radiation dose estimates in humans for (11)C-acetate whole-body PET. J Nucl Med.
21 Gropler R.J., Siegel B.A., Geltman E.M. (1991). Myocardial uptake of carbon-11-acetate as an indirect estimate of regional myocardial blood flow. J Nucl Med.
22 Sciacca R.R., Akinboboye O., Chou R.L., Epstein S., Bergmann S.R. (2001). Measurement of myocardial blood flow with PET using 1-11C-acetate. J Nucl Med.